# N-(4-(6-(Isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-N-methyl-4-[^11^C]methylbenzamide

Chemical name: | N-(4-(6-(Isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-N-methyl-4-[^11^C]methylbenzamide
Abbreviated name: | [^11^C]ITDM, [^11^C]4
Synonym:
Agent category: | Compound
Target: | Metabotropic glutamate receptor subtype 1 (mGluR1)
Target category: | Receptor
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=23194448)]

Glutamate is a major excitatory neurotransmitter at neuronal synapses in the central nervous system (CNS) (1, 2). Glutamate produces excitatory effects by acting on cell-surface ionotropic glutamate or metabotropic glutamate receptors (mGluRs). The mGluRs are GTP-binding protein (G-protein)–coupled receptors that play important roles in regulating the activity of many synapses in the CNS, and many neuronal projection pathways contain mGluRs. There are eight mGluR subtypes, which are further subdivided into groups I, II, and III. The group I receptors include mGluR1 and mGluR5, and they are found predominantly in postsynaptic locations. mGluR1 is found in moderate to high density in the cerebellum, caudate, putamen, thalamus, cingulate cortex, and hippocampus, with low density in the pons. mGluR5 is usually found in moderate to high density in the frontal cortex, caudate, putamen, nucleus accumbens, olfactory tubercle, and hippocampus, with low density in the cerebellum. mGluR1 and mGluR5 are positively coupled to phospholipase C in the regulation of neuronal excitability (3). Dysfunction of mGluR1 and mGluR5 is implicated in a variety of diseases in the CNS, including anxiety, depression, schizophrenia, Parkinson’s disease, and drug addiction or withdrawal (2, 4).

Positron emission tomography (PET) radioligands targeting mGluR5 can visualize and analyze mGluR5 expression in normal physiological and pathological conditions (4-8). However, only a few mGluR1 ligands have been studied. N-(4-(6-(Isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-N-methyl-4-methylbenzamide (ITDM) was shown to be a selective mGluR1 antagonist with nanomolar affinity (K_i_ = 13.6 nM), with little inhibition of mGluR5 (9). Fujinaga et al. (9) labeled ITDM with ^11^C to prepare N-(4-(6-(isopropylamino)pyrimidin-4-yl)-1,3-thiazol-2-yl)-N-methyl-4-[^11^C]methylbenzamide ([^11^C]ITDM) for use with in vivo PET imaging of mGluR1 distribution in rat and monkey brains.

### Related Resource Links:

- Chapters in MICAD (mGluR1 (http://www.ncbi.nlm.nih.gov/books?Db=books&Cmd=DetailsSearch&Term=mGluR1+AND+micad%5Bbook%5D), mGluR5 (http://www.ncbi.nlm.nih.gov/books?term=mGluR5%20AND%20micad%5Bbook%5D))
- Gene information in NCBI (mGluR1 (http://www.ncbi.nlm.nih.gov/gene/2911), mGluR5 (http://www.ncbi.nlm.nih.gov/gene/2915))
- Articles in Online Mendelian Inheritance in Man (OMIM) (mGluR1 (http://omim.org/entry/604473), mGluR5 (http://www.ncbi.nlm.nih.gov/omim/604102))
- Clinical trials (mGluR1 (http://www.clinicaltrials.gov/ct2/results?term=mGluR1), mGluR5 (http://www.clinicaltrials.gov/ct2/results?term=mglur5))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=23194448%20and%20synthesis)]

Fujinaga et al. (9) synthesized [^11^C]ITDM by methylation of the arylstannane precursor with [^11^C]MeI (prepared with [^11^C]CO_2_) using an automated synthesizer for 5 min at 80°C. Subsequent separation with high-performance liquid chromatography produced a radiochemical purity >99%. Average radiochemical yield was 19 ± 9% (n = 11) based on [^11^C]CO_2_. The specific activity of [^11^C]ITDM was 70–170 GBq/µmol (1.89–4.59 Ci/µmol) at the end of synthesis. The total synthesis time was <31 min from the end of bombardment.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=23194448%20and%20in%20vitro)]

In vitro binding affinity of ITMM was determined with rat brain homogenates using [^18^F]fluoro-N-[4-[6-(isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methylbenzamide ([^18^F]FITM) as the mGluR1 radioligand (9). The K_i_ values were 13.6 ± 3.4 nM and 5.4 ± 1.2 nM for ITDM and FITM, respectively. Both agents showed IC_50_ values >10,000 nM for mGluR5. ITDM (LogD 1.74) was found to be slightly more lipophilic than FITM (LogD 1.45).

In vitro [^11^C]ITDM autoradiographic imaging studies were performed on rat brain sections (9). [^11^C]ITDM bound heterogeneously to the brain sections, with the highest accumulation of radioactivity in the mGluR1-rich cerebellum, followed by the thalamus, hippocampus, striatum, and cerebral cortex, with the lowest radioactivity in the pons. ITDM and JNJ-16259685 (1,000 nM), both mGluR1 antagonists, blocked radioactivity to homogeneity in the brain sections.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=23194448%20and%20rodentia)]

Fujinaga et al. (9) performed ex vivo biodistribution studies in mice (n = 4/group) at 1–90 min after intravenous injection of 4.8 MBq (0.13 mCi) [^11^C]ITDM (0.04 nmol). The radioactivity levels in most tissues were highest at 1–5 min and decreased gradually thereafter. The highest accumulation at 5 min was observed in the small intestine (66.76% injected dose/gram (ID/g)), followed by the liver (11.38% ID/g), kidney (4.41% ID/g), brain (2.58% ID/g), lung (2.56% ID/g), heart (1.28% ID/g), blood (1.27% ID/g), muscle (0.96% ID/g), and spleen (0.93% ID/g). The accumulation in the brain remained high at 1.99% ID/g and 1.59% ID/g at 15 min and 30 min, respectively. No blocking studies were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=23194448%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=23194448%20and%20%28primate%20not%20human%29)]

Fujinaga et al. (9) performed dynamic PET imaging studies for 90 min in a male rhesus monkey after intravenous injection of 185–220 MBq (5.0–5.9 mCi) [^11^C]ITDM (5–6 nmol). Blocking studies were performed with injection of excess ITDM (1 mg/kg) or mGluR1 antagonist JNJ-16259685 (3 mg/kg) just before injection of the tracer in the same monkey two weeks later. Baseline tissue time-activity curves revealed high accumulation of radioactivity that peaked at 15–30 min in the cerebellum, with moderate radioactivity in the cingulate cortex, thalamus, and striatum and low radioactivity in the pons. The radioactivity declined in all brain regions after the peaks. The maximum standard uptake values in the cerebellum, cingulate cortex, and thalamus were 1.2, 0.9, and 0.8 at ~20 min after injection of [^11^C]ITDM, respectively. Pretreatment with ITDM and JNJ-16259685 reduced the levels of radioactivity to that of the whole brain. Logan graphic analysis was used to estimate the distribution volume ratio (DVR) values under the equilibrium state. The DVR values were 4.3, 2.6, 2.0, 1.8, 1.5, 1.5, and 1.0 for the cerebellum, cingulate cortex, thalamus, hippocampus, caudate, putamen, and pons, respectively.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=23194448%20and%20human)]

No publication is currently available.

## References

1 Pin J.P., Duvoisin R. (1995). The metabotropic glutamate receptors: structure and functions. Neuropharmacology.
2 Ferraguti F., Crepaldi L., Nicoletti F. (2008). Metabotropic glutamate 1 receptor: current concepts and perspectives. Pharmacol Rev.
3 Abe T., Sugihara H., Nawa H., Shigemoto R., Mizuno N., Nakanishi S. (1992). Molecular characterization of a novel metabotropic glutamate receptor mGluR5 coupled to inositol phosphate/Ca2+ signal transduction. J Biol Chem.
4 Gasparini F., Lingenhohl K., Stoehr N., Flor P.J., Heinrich M., Vranesic I., Biollaz M., Allgeier H., Heckendorn R., Urwyler S., Varney M.A., Johnson E.C., Hess S.D., Rao S.P., Sacaan A.I., Santori E.M., Velicelebi G., Kuhn R. (1999). 2-Methyl-6-(phenylethynyl)-pyridine (MPEP), a potent, selective and systemically active mGlu5 receptor antagonist. Neuropharmacology.
5 Ametamey S.M., Kessler L.J., Honer M., Wyss M.T., Buck A., Hintermann S., Auberson Y.P., Gasparini F., Schubiger P.A. (2006). Radiosynthesis and preclinical evaluation of 11C-ABP688 as a probe for imaging the metabotropic glutamate receptor subtype 5. J Nucl Med.
6 Ametamey S.M., Treyer V., Streffer J., Wyss M.T., Schmidt M., Blagoev M., Hintermann S., Auberson Y., Gasparini F., Fischer U.C., Buck A. (2007). Human PET studies of metabotropic glutamate receptor subtype 5 with 11C-ABP688. J Nucl Med.
7 Baumann C.A., Mu L., Johannsen S., Honer M., Schubiger P.A., Ametamey S.M. (2010). Structure-activity relationships of fluorinated (E)-3-((6-methylpyridin-2-yl)ethynyl)cyclohex-2-enone-O-methyloxime (ABP688) derivatives and the discovery of a high affinity analogue as a potential candidate for imaging metabotropic glutamate recepors subtype 5 (mGluR5) with positron emission tomography (PET). J Med Chem.
8 Honer M., Stoffel A., Kessler L.J., Schubiger P.A., Ametamey S.M. (2007). Radiolabeling and in vitro and in vivo evaluation of [(18)F]-FE-DABP688 as a PET radioligand for the metabotropic glutamate receptor subtype 5. Nucl Med Biol.
9 Fujinaga M., Yamasaki T., Maeda J., Yui J., Xie L., Nagai Y., Nengaki N., Hatori A., Kumata K., Kawamura K., Zhang M.R. (2012). Development of N-[4-[6-(Isopropylamino)pyrimidin-4-yl]-1,3-thiazol-2-yl]-N-methyl-4-[(11)C]methy lbenzamide for Positron Emission Tomography Imaging of Metabotropic Glutamate 1 Receptor in Monkey Brain. J Med Chem.